# ^99m^Tc-Ethylenedicysteine-C225

Chemical name: | ^99m^Tc-Ethylenedicysteine-C225
Abbreviated name: | ^99m^Tc-EC-C225
Synonym: | ^99m^Tc-EC-cetuximab
Agent category: | Chimeric monoclonal antibody
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Single photon emission computed tomography (SPECT)
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=41327732), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22cetuximab%22%5BSubstance%20Name%5D)]

Epidermal growth factor (EGF) is a 53-amino acid cytokine (6.2 kDa) secreted by ectodermic cells, monocytes, kidneys and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF receptor (EGFR) is a transmembrane protein with an intracellular tyrosine kinase present on most cells. EGFR is overexpressed on many solid tumor cells such as breast, non-small-cell lung, head and neck, and colon cancer (2-4). The high level of EGFR expression on cancer cells is associated with a poor prognosis (5-7). Inhibition of EGF receptor functions by C225 (also known as centuximab), an anti-EGFR chimeric monoclonal antibody, has been shown to inhibit tumor angiogenesis, growth and metastasis (8, 9). ^99m^Tc-EC-C225 was developed as a single photon emission computed tomography (SPECT) tracer for imaging EGFR expression on solid tumors (10, 11).

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/books?term=EGFR%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (Cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EC-C225%5BAll%20Fields%5D)]

L,L-Ethylenedicysteine (EC) was conjugated to C225-NH_2_ using sulfo-N-hydroxysulfosuccinimide (10) to form EC-C225, which was purified by G-25 column chromatography. A radiochemical purity of 100% was achieved, as measured by high-performance liquid chromatography (HPLC) analysis. The specific activity was calculated to be about 74 MBq/μmol (2 Ci/μmol) before in vivo injection to rats.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EC-C225%5BAll%20Fields%5D%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

Three human breast cancer lines (A431 - high EGFR expression, MDA231 - medium, and MDA453 - low) with different EGFR levels were used to study the integrity of EC-C225. Western immunoblotting and immunoprecipitation studies showed that there were no differences between EC-C225 and C225 in binding to EGFR in these three cell lines (10). EC-C225 induced apoptosis in DiFi cells to the same extent as C225. There was a 4% uptake of ^99m^Tc-EC-C225 (0.074 MBq, 2 μCi) by A431 cells at the end of 2 h incubation. There was only a marginal uptake by MDA231 cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EC-C225%5BAll%20Fields%5D%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29)]

Rats bearing mammary adenocarcinoma 13762 NF received intravenous injections of 0.74 MBq/rat (20 μCi/rat) of ^99m^Tc-EC-C225 or ^99m^Tc-EC (10). The organs with the major uptake of ^99m^Tc-EC-C225 were the kidneys (14.8% injected dose/g (ID/g)) and liver (0.72% ID/g) at 2 h. The tumor had an uptake of 0.31% ID/g versus 0.12% ID/g for ^99m^Tc-EC. A tumor/muscle ratio of about 8 was estimated for ^99m^Tc-EC-C225 as compared with 4 for ^99m^Tc-EC. Pretreatment (30 min before tracer injection) of tumor-bearing rats with 100-fold excess of unlabeled C225 decreased the ^99m^Tc-EC-C225 tumor/muscle ratio to about 4 (background) at 2 h after injection of the tracer.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EC-C225%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EC-C225%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EC-C225%20AND%20human)]

Human dosimetry of ^99m^Tc-EC-C225 was determined from blood samples and SPECT images in 6 patients with head and neck carcinoma after intravenous injection of 925 MBq (25 mCi) (11). High uptake in the kidneys, spleen, liver, and gallbladder was observed. The effective dose equivalent was estimated to be 0.006 mSv/MBq (22 mrem/mCi). The organ that received the highest dose was the kidneys (0.0274 mGy/MBq or 0.1014 rad/mCi), followed by the spleen (0.0214 mGy/MBq or 0.0793 rad/mCi), liver (0.0157 mGy/MBq or 0.058 rad/mCi), and gallbladder (0.0059 mGy/MBq or 0.0219 rad/mCi).

## NIH Support

CA16672, P01 CA06294

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
3 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
4 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
5 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
6 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
7 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
8 Fan Z., Masui H., Altas I., Mendelsohn J. (1993). Blockade of epidermal growth factor receptor function by bivalent and monovalent fragments of 225 anti-epidermal growth factor receptor monoclonal antibodies. Cancer Res.
9 Kim E.S., Khuri F.R., Herbst R.S. (2001). Epidermal growth factor receptor biology (IMC-C225). Curr Opin Oncol.
10 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
11 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.